# Trastuzumab complexed to near-infrared fluorophore indocyanine green

Chemical name: | Trastuzumab complexed to near-infrared fluorophore indocyanine green
Abbreviated name: | Tra-ICG
Synonym:
Agent Category: | Monoclonal antibody
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Optical: near-infrared (NIR) fluorescence
Source of signal / contrast: | Indocyanine green
Activation: | Yes
Studies: | - In vitro; - Rodents | Proposed structure of Trastuzumab-Indocyanine green conjugate..

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+indocyanine+green)]

The technique of non-invasive optical imaging is based on the principle that when a dye is exposed to light it absorbs energy and is elevated from the steady state to a high-energy state. To return to its normal, low-energy state, the molecule releases energy in the form of photons with wavelengths that are either in the visible (400–700 nm) or the near infrared (NIR; 700–900 nm) range (1). Although both types of dyes can be used for imaging, in general, NIR agents are favored over those functional in the visible range because fluorescence from NIR probes can be detected in deep tissue, have low autofluorescence, and generate low background signals because tissues do not absorb in the NIR wavelength range (2). Among the various NIR agents, only one, indocyanine green (ICG; also known as IR-125 or Cardiogreen), with absorption at ~780 nm and emission at ~820 nm, is approved by the United States Food and Drug Administration (US FDA) for clinical applications (3) and is under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications. ICG is a tricarbocyanine dye that is fluorescent only in the free state and easily binds to proteins through non-covalent linkages (such as ionic, hydrophobic, electrostatic, or hydrogen bonds). When bound to proteins ICG is non-fluorescent, but on dissociation from the protein complex it reverts to the fluorescent state and the signal has been shown to be suitable for in vivo imaging in small animals (4).

The human epidermal growth factor receptor (HER; it has several isoforms: HER1, HER2, HER3, and HER4) plays an important role in the development and progression of cancers (5-7). The HER mediates its activity through a tyrosine kinase signaling pathway, and on binding to a ligand the receptor signaling pathway is activated, which promotes cell growth and division. Once activated the receptor-ligand complex is internalized by the cell for enzymatic digestion in the lysosome (8). Because of its role in the cancer process, several commercially available humanized monoclonal antibodies (MAb) directed toward HER, including trastuzumab (Tra), are approved by the US FDA to treat cancers. Tra targets the HER2 receptor and is used as the primary agent or as an adjuvant for the treatment of breast cancer in the clinical setting (9). It is also being investigated in several clinical trials (http://clinicaltrials.gov/ct2/results?term=trastuzumab) to treat other neoplasms.

The characteristic properties of ICG (fluorescence in an unbound state) and the HER (internalization by the cell) prompted Ogawa et al. to develop an imaging probe for cancer by complexing ICG to Tra (Tra-ICG) (4). The investigators used the Tra-ICG complex to image cells that express the HER2 receptor under in vitro conditions and showed that the complex could also be used for the imaging of HER2-expressing xenograft tumors in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+synthesis)]

The synthesis of Tra-ICG was described by Ogawa et al. (4). ICG-N-hydroxysulfosuccinimide ester (ICG-sulfo-OSu) and Tra were obtained from commercial sources. Tra was incubated with ICG-sulfo-OSu (Tra:ICG ratio was either 1:1 or 1:5) in phosphate buffer (pH 8.5) for 30 min at room temperature. The Tra-ICG complex was purified on a PD-10 Sephadex G50 column with phosphate-buffered saline (PBS; pH not reported) as the elution buffer. With the reaction conditions used to generate the MAb-ICG complex, either one or five ICG molecules (Tra-ICG(1:1) or Tra-ICG(1:5), respectively) were reported to be bound to each Tra molecule, respectively. To determine specificity of the Tra-ICG complex, another MAb, panitumumab (Pan), which specifically binds to HER1, was complexed with ICG (Pan-ICG) and purified as described above.

For use as a control, a human polyclonal IgG-Cy5.5 complex was also synthesized in the manner described above. The storage conditions and stability of the MAb-ICG complexes were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+in+vitro)]

Fluorescence imaging with the Tra-ICG complex was investigated in HER2 gene-transfected NIH3T3 (3T3/HER2+) cells (4). The cells were grown on a glass-bottomed tissue culture well and exposed to the Tra-ICG(1:1) or Tra-ICG(1:5) complex for 1 and 8 h at 37^o^C. The cells were then washed with PBS and examined under a fluorescent microscope. No fluorescence was observed in cells exposed to Tra-ICG(1:1) at either time point. Fluorescence was apparent with both complexes at 8 h, indicating that the signal was obtained only after internalization of the MAb-ICG complex followed by degradation of the MAb and release of the ICG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+rodentia)]

Xenograft tumors were generated with 3T3/HER2+ cells in the left and right flank and the right buttock of three mice for imaging studies (4). The tumors were visible on the mice 14 to 18 days after the cell injection. The Tra-ICG (n = 1 animal) or the Pan-ICG (n = 1 animal) complex was administered intravenously to the animals through the tail vein. Fluorescent imaging was performed on the mice 4 days after the Tra-ICG or Pan-ICG injection. To confirm the presence of tumor histology, an ex vivo histological examination of the tumors was performed using the hematoxylin and eosin (H&E) stain of embedded tumor sections. Only animals injected with Tra-ICG generated a fluorescent signal in the 3T3/HER2+ cell tumors and were imaged under these conditions, indicating that the Tra-ICG complex bound specifically to the HER2+ tumors. A histological examination of the tumors was reported to show expected differences between the tumors.

To confirm the specificity of the Tra-ICG complex under in vivo conditions, mice bearing the NIH3T3/HER2+ tumors were co-injected with Tra-ICG or the Pan-ICG complex along with the polyclonal IgG-Cy5.5 conjugate (4). Imaging was performed on these animals 4 days after the injection. An ex vivo histological examination of the tumors was also performed with the H&E stain as described above. Under these conditions, all tumors could be imaged because the IgG-Cy5.5 complex generated similar fluorescence (red) in all the tumors. Using commercially available software, separation of the respective fluorescent signals obtained from ICG and Cy5.5 showed that the ICG signal was visible only in the HER2+ cell tumors, but the Cy5.5 fluorescence was detected in all tumors in the mice. This again confirmed that the Tra-ICG complex was specific for the HER2+ tumors. No competition studies using animals pretreated with Tra were reported.

With observations from this study, the investigators concluded that the Tra-ICG complex technique could probably be adapted for tumor imaging in humans during surgery. However, they cautioned that the Tra-ICG complex could have a different toxicity compared with individual components of the complex, and extensive clinical testing of Tra-ICG would have to be performed before its application in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+Human+Studies)]

No references are currently available.

## References

1 Sharma R., Wendt J.A., Rasmussen J.C., Adams K.E., Marshall M.V., Sevick-Muraca E.M. (2008). New horizons for imaging lymphatic function. Ann N Y Acad Sci.
2 Luker G.D., Luker K.E. (2008). Optical imaging: current applications and future directions. J Nucl Med.
3 Sakka S.G. (2007). Assessing liver function. Curr Opin Crit Care.
4 Ogawa, M., N. Kosaka, P.L. Choyke, and H. Kobayashi, In vivo Molecular Imaging of Cancer with a Quenching Near-Infrared Fluorescent Probe Using Conjugates of Monoclonal Antibodies and Indocyanine Green. Cancer Res, 2009
5 Weber J., McCormack P.L. (2008). Panitumumab: in metastatic colorectal cancer with wild-type KRAS. BioDrugs.
6 Mehra R., Cohen R.B., Burtness B.A. (2008). The role of cetuximab for the treatment of squamous cell carcinoma of the head and neck. Clin Adv Hematol Oncol.
7 Hall P.S., Cameron D.A. (2009). Current perspective - trastuzumab. Eur J Cancer.
8 Woodman P. (2009). ESCRT proteins, endosome organization and mitogenic receptor down-regulation. Biochem Soc Trans.
9 Simonds H.M., Miles D. (2007). Adjuvant treatment of breast cancer: impact of monoclonal antibody therapy directed against the HER2 receptor. Expert Opin Biol Ther.